# [^99m^Tc]-Mercaptoacetyldiglycyl-1,5-diaminopentylene hypericincarboxamide

Chemical name: | [^99m^Tc]-Mercaptoacetyldiglycyl-1,5-diaminopentylene hypericincarboxamide
Abbreviated name: | [^99m^Tc]-Hypericin
Synonym: | [^99m^Tc]-13
Agent Category: | Compound
Target: | Necrotic tissue
Target Category: | Binding to unknown cell membrane component(s)
Method of detection: | Single-photon emission computed tomography, planar gamma imaging
Source of Signal/Contrast: | [^99m^Tc]
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D)]

Hypericin, a polycyclic polyaromatic quinone with photosensitive properties, is found in the Saint John's wort plant (Hypericum perforatum), has a chemical structure that is similar to some porphyrin derivatives, and has been investigated for the photodynamic detection, diagnosis, and treatment of various cancers (1, 2). Because porphyrins bind in vitro primarily to the necrotic tissue found in neoplastic tumors, investigators have evaluated the use of hypericin derivatives labeled with radioactive iodine (^123^I), such as mono-[^123^I]iodohypericin ([^123^I]MIH) and mono-[^123^I]iodohypericin monocarboxylic acid ([^123^I]MIHA), for the detection of necrotic tissue in the myocardium after an acute myocardial infarction and in the necrosed liver (3-7). Although the ^123^I-labeled derivatives of hypericin were shown to be suitable for the detection of necrotic tissue, Fonge et al. thought a technetium (^99m^Tc)-labeled derivative of hypericin would be more suitable for the imaging of necrosed tissue because this radio-metal has better availability than ^123^I (8).

To achieve the labeling of hypericin with ^99m^Tc, hypericin was first conjugated to a bifunctional chelating agent, mercaptoacetyldiglycyl-1,5-diaminopentylene, and then it was linked to the tracer metal to obtain [^99m^Tc]-mercaptoacetyldiglycyl-1,5-diaminopentylene hypericin carboxamide, designated as ^99m^Tc-13 by the investigators (8). The labeled compound was subsequently investigated for biodistribution in normal mice and evaluated for the detection of necrotic tissue in rats with a reperfused hepatic infarct.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+labeled+hypericin+synthesis)]

The synthesis of ^99m^Tc-labeled hypericin was detailed by Fonge et al. (8). Briefly, S-benzoylmercaptoacetylglycylglycine and N-hydroxysuccinimide (NHS) were dissolved in methylene chloride (MC) and dimethylformamide (DMF) and cooled to 0°C; N,N'-dicyclohexylcarbodiimide in MC was added dropwise to the solution. The mixture was stirred for 1 h at 0°C and for another 16 h at room temperature (RT). The resulting precipitate was washed with a MC/DMF mixture, and the solvent was evaporated under reduced pressure to obtain N-succinimidyl-S-benzoylmecrcaptoacetylglycylglycine. The benzoylmercaptoacetyl compound was recrystallized from ethyl acetate as a white powder with 84% yield.

A solution of the benzoylmercaptoacetyl compound in tetrahydrofuran (THF) was added to a mixture of N-di-tertiary-butyldicarbonate-1,5-diaminopentane and triethylamine also in THF and stirred overnight at RT. The solvent was evaporated from the mixture and water was added, resulting in the formation of a white precipitate, S-benzoylmercaptoacetyldiglycyl-1-amino-5-N-di-tertiary-butyldicarbonate-aminopentane, with a yield of 93.3%. The aminopentane was dissolved in trifluoroacetic acid in a flask under nitrogen at –5°C and stirred at this temperature for 20 min, followed by stirring at RT for another 40 min. The trifluoroacetic acid was evaporated azeotropically under reduced pressure with hexane to obtain a brown oil. Upon addition of acetonitrile to the oil, a precipitate, S-benzoylmercaptoacetyldiglycyl-1,5-diaminopentane, was obtained.

Protohypericin monocarboxylic acid was obtained as described by Fonge et al. (8), dissolved in THF along with NHS, and cooled to 0°C. Subsequently N,N’-dicyclohexylcarbodiimide in THF was added dropwise, and the mixture was stirred at 0°C for 1 h and then overnight at RT. The dicyclohexyl urea was filtered, and the filtrate was evaporated to yield a dark purple compound, N-succinimidyl protohypericin monocarboxylic acid, with a yield of 70%.

The monocarboxylic acid and diisopropylethylamine were dissolved in THF, and a solution of S-benzoylmercaptoacetyldiglycyl-1,5-diaminopentane in DMF was added to it. The mixture was stirred for 15 h at RT, and the solvents were evaporated under reduced pressure to yield a crude S-benzoylmercaptoacetyldiglycyl-1,5-diaminopentylene protohypericin-carboxamide. The carboxamide was purified with reverse-phase high-performance liquid chromatography (RP-HPLC) with a yield of 60%.

Removal of the S-benzoyl protecting group, followed by the ^99m^Tc-labeling of S-benzoylmercaptoacetyldiglycyl-1,5-diaminopentylene protohypericin-carboxamide, was performed in a single reaction vial (8). For this, the carboxamide was dissolved in ethanol and buffered with phosphate buffer to pH 10.0; this was followed by the consecutive addition of sodium-potassium tartrate, stannous chloride dihydride, and sodium pertechnetate (TcO_4_^-^). The mixture was heated at 100°C for 20 min and irradiated for 30 min with a 400-W halogen lamp to obtain [^99m^Tc]-hypericin. The labeled hypericin was then purified with RP-HPLC. The solvents were evaporated at 40°C with a gentle flush of nitrogen, and [^99m^Tc]-hypericin was formulated in water/polyethylene glycol 400 for biodistribution studies. The specific activity, radiochemical yield and purity, and stability of [^99m^Tc]-hypericin were not provided by the investigators (although the publication mentioned that the stability of [^99m^Tc]-hypericin was determined at various time points with RP-HPLC) (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+hypericin+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+hypericin+rodentia)]

The biodistribution of [^99m^Tc]-hypericin was investigated in normal Naval Medical Research Institute mice (8). The animals were injected with the radiochemical through the tail vein and euthanized 30 min, 4 h, and 24 h after injection (n = 4 animals per time point). The organs were removed and weighed, and the radioactivity in all organs, including blood, was counted. The label was slowly cleared through the hepatobiliary route, which resulted in the appearance of 33% and 63% of the injected dose (% ID) in the intestines at 4 h and 24 h after injection, respectively. Blood clearance of [^99m^Tc]-hypericin was reported to be rapid with only 0.5% ID/g remaining at 30 min after injection. This indicated that the radiocompound had a faster clearance rate than the previously published ^123^I-labeled hypericin derivatives (4-6). Similar to [^123^I]MIH and [^123^I]MIHA, the uptake of [^99m^Tc]-hypericin was observed to be high in the liver, but the ^99m^Tc derivative was cleared faster from this organ than the ^123^I-labeled compounds (4-6, 8). Little clearance of [^99m^Tc]-hypericin was detected through the urinary route.

The visualization of necrotic tissue with [^99m^Tc]-hypericin was performed in rats (n = 4 animals) with reperfused hepatic infarction (8). The animals were injected with [^99m^Tc]-hypericin through the tail vein and euthanized 4 h and 24 h after injection (n = 2 animals per time point). The livers were removed from the animals, and the necrotic and viable tissues were separated, thoroughly washed with saline, and frozen. Serial sections of the frozen tissue were cut and mounted on slides for autoradiography, after which the samples were stained with hematoxylin and eosin for microscopic confirmation of the presence of necrotic tissue. Uptake of the label by both the necrotic tissues and viable tissues was also confirmed by gamma countingand autoradiography. The ratios of necrotic tissue radioactivity to viable hepatic tissue radioactivity were 0.5 and 0.8 at 4 and 24 h after injection, respectively. These ratios were significantly lower than those seen with [^123^I]MIHA for necrotic or viable liver tissues (4, 8). On the basis of the necrotic/non-necrotic tissue uptake ratios, the investigators concluded that chelation of ^99m^Tc reduced the affinity of hypericin for necrotic tissue, and that [^99m^Tc]-hypericin was not a suitable agent for the detection of such tissue.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+hypericin+non+primate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+hypericin+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc+hypericin+human+studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Kiesslich T., Krammer B., Plaetzer K. (2006). Cellular mechanisms and prospective applications of hypericin in photodynamic therapy. Curr Med Chem.
2 Zaak D., Karl A., Knuchel R., Stepp H., Hartmann A., Reich O., Bachmann A., Siebels M., Popken G., Stief C. (2005). Diagnosis of urothelial carcinoma of the bladder using fluorescence endoscopy. BJU Int.
3 Bormans G., Huyghe D., Christiaen A., Verbeke K., de Groot T., Vanbilloen H., de Witte P., Verbruggen A. (2004). Preparation, analysis and biodistribution in mice of iodine-123 laballed derivatives of hypericin. . J Label Comp Radiopharm.
4 Fonge H., Jin L., Wang H., Ni Y., Bormans G., Verbruggen A. (2007). Synthesis and preliminary evaluation of mono-[123I]iodohypericin monocarboxylic acid as a necrosis avid imaging agent. Bioorg Med Chem Lett.
5 Fonge H., Van de Putte M., Huyghe D., Bormans G., Ni Y., de Witte P., Verbruggen A. (2007). Evaluation of tumor affinity of mono-[(123)I]iodohypericin and mono-[(123)I]iodoprotohypericin in a mouse model with a RIF-1 tumor. Contrast Media Mol Imaging.
6 Fonge H., Vunckx K., Wang H., Feng Y., Mortelmans L., Nuyts J., Bormans G., Verbruggen A., Ni Y. (2008). Non-invasive detection and quantification of acute myocardial infarction in rabbits using mono-[123I]iodohypericin {micro}SPECT. Eur Heart J.
7 Ni Y., Huyghe D., Verbeke K., de Witte P.A., Nuyts J., Mortelmans L., Chen F., Marchal G., Verbruggen A.M., Bormans G.M. (2006). First preclinical evaluation of mono-[123I]iodohypericin as a necrosis-avid tracer agent. Eur J Nucl Med Mol Imaging.
8 Fonge H., Jin L., Wang H., Bormans G., Ni Y., Verbruggen A. (2008). Synthesis and preliminary biological evaluation of a 99mTc-labeled hypericin derivative as a necrosis avid imaging agent. J Label Comp Radiopharm.